# ^18^F-Fluoroethyl triazole-βAG-[(D)-Phe^1^-c(Cys^2^-Tyr^3^-(D)-Trp^4^-Lys^5^-Thr^6^-Cys^7^)Thr^8^]

Chemical name: | ^18^F-Fluoroethyl triazole-βAG-[(D)-Phe^1^-c(Cys^2^-Tyr^3^-(D)-Trp^4^-Lys^5^-Thr^6^-Cys^7^)Thr^8^] | [image]
Abbreviated name: | ^18^F-FET-βAG-TOCA | [image]
Synonym: | [^18^F]-5b | [image]
Agent Category: | Peptides | [image]
Target: | Somatostatin receptors (mainly SSTR-2) | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Schematic structure of ^18^F-FET-βAG-TOCA by Iddon et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gastroenteropancreatic%20neuroendocrine%20tumours%20and%20molecular%20imaging)]

The ^18^F-labeled fluoroethyl triazole (FET)-βAG-[(D)-Phe^1^-c(Cys^2^-Tyr^3^-(D)-Trp^4^-Lys^5^-Thr^6^-Cys^7^)Thr^8^] (TOCA or Tyr^3^-octreotide), abbreviated as ^18^F-FET-βAG-TOCA, is a Tyr^3^-octreotate analog that was synthesized for positron emission tomography of gastroenteropancreatic neuroendocrine tumors (GEP-NETs) by targeting somatostatin receptors (SSTR, mainly SSTR-2) (1, 2).

GEP-NETs are a class of fairly rare tumors with secretion of various peptides and neuroamines. Although significant progress has been made in the understanding of the molecular events underlying these tumors, it is challenging for the early diagnosis, new target identification, and effective management of these tumors (3, 4). In 1989, Krenning et al. first introduced the use of ^123^I-labeled Tyr^3^-octreotide for in vivo imaging of SSTR-expressing GEP-NETs (5). However, this agent exhibited high nonspecific accumulation in the liver and intestine, which can obscure the detection of early-stage GEP-NETs. In 1993, Krenning et al. developed another ^111^In-labeled somatostatin analog, [^111^In-DTPA^0^]octreotide (6), and since then this agent has become the gold standard in nuclear imaging for patients with GEP-NETs (6, 7). An obvious disadvantage for [^111^In-DTPA^0^]octreotide is that imaging has to be performed 1–2 days after its injection to ensure sufficient contrast (half-life of ^111^In, 2.8 days). Recently, studies have been mainly focused on two aspects: searching for new analogs that would have a better affinity profile compared with [^111^In-DTPA^0^]octreotide, and developing effective methods for other radionuclide labeling (4, 7, 8).

In general, positron-emitting radionuclide-labeled analogs share excellent imaging quality with better spatial resolution compared to the imaging quality of γ-emitting analogs. One representative agent is [^68^Ga-DOTA^0^,Tyr^3^]octreotide (^68^Ga-DOTATOC), which is the first ^68^Ga-labeled somatostatin analog that is studied in patients (9). ^18^F-Labeled analogs, such as the glycosylated analog Gluc-Lys([^18^F]FP)-TOCA, which is comparable with ^68^Ga-DOTATOC in in vivo imaging, have also been studied (10). However, the preparation of Gluc-Lys([^18^F]FP)-TOCA is time-consuming. Iddon et al. labeled a novel class of alkyne-linked Tyr^3^-octreotate analogs with a copper-catalyzed azide-alkyne cycloaddition reaction (CuAAC) to form a 1,4-substituted triazole using the reagent [^18^F]2-fluoroethyl azide (1). The ^18^F-labeling process is fast and efficient. With this labeling method, investigators have identified two lead alkyne-linked Tyr^3^-octreotate analogs, G-TOCA and βAG-TOCA (1). Both lead analogs were highly reactive in the CuAAC reaction, showing complete conversion to the [^18^F]2-fluoroethyl triazole-linked Tyr^3^-octreotate analogs FET-G-TOCA and FET-βAG-TOCA under mild conditions and with short synthesis times (5 min at 20°C). Leyton et al. further tested these ^18^F-labeled analogs for their receptor binding and in vivo tumor imaging (2). This chapter summarizes the data obtained with these analogs (1, 2).

### Related Resource Links:

SSTR-targeting imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=somatostatin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=Somatostatin%20Receptors) and protein (http://www.ncbi.nlm.nih.gov/protein/?term=Somatostatin%20Receptors) sequences of SSTR

SSTR-targeted clinical trials (http://clinicaltrials.gov/ct2/results?term=somatostatin+receptor)

NCBI resources (http://www.ncbi.nlm.nih.gov/guide/all/)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=iddon%20L%20and%202011)]

Iddon et al. labeled five Tyr^3^-octreotate analogs (compound 1b–5b) and one scrambled peptide (compound 6b) with [^18/19^F]2-fluoroethyl azide using click chemistry (1). Compounds 1b and 2b were the PEGylated forms of 3b and 4b. All radiotracers were successfully prepared with >98% radiochemical purity. The total synthesis time for each compound was ~1.5 h. The ^19^F-labeled analogs were used for in vitro analysis of SSTR subtype binding. The ^18^F-labeled analogs were used for other studies. The molecular weights (MW), radiochemical yields (RCY), specific radioactivity (SR) (GBq/µmol), and octanol/PBS partition coefficients (Log D) of the tracers are shown in Table 1 (1, 2).

Table 1: Characteristics of the Tyr^3^-octreotate analogs

Compound | Synonym | MW | RCY (%) | | SR (GBq/µmol) | Log D ^18^F-Labeled
Compound | Synonym | MW | ^19^F-Labeled | ^18^F-Labeled | SR (GBq/µmol) | Log D ^18^F-Labeled
FET-G-PEG-TOCA | 1b | 1,604.8 | 35 | 40 | 4.8 | −2.68
FETE-PEG-TOCA | 2b | 1,575.8 | 44 | 52 | 5.9 | −2.77
FET-G-TOCA | 3b | 1,269.4 | 37 | 50 | 5.9 | −1.83
FETE-TOCA | 4b | 1,240.4 | 56 | 51 | 8.4 | −1.5
FET-βAG-TOCA | 5b | 1,340.5 | 29 | 66 | 18.7 | −2.26
FET-βAG-[W-c-(CTFTYC)K] | 6b | 1,340.5 | 38 | 64 | 12.3 | −1.14

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=iddon%20L%20and%202011)]

Leyton et al. evaluated the binding affinity of ^19^F-labeled Tyr^3^-octreotate analogs for SSTR-2 and SSTR-4 in SSTR-2– or SSTR-4–expressing Chem-1 cells with a fluorometric imaging plate reader assay (2) All analogs exhibited agonist activity on SSTR-2, with the scrambled peptide (compound 6b) having expectedly poor affinity (Table 2). The affinity of the ligands (half-maximal effective concentration) ranged from 4 nM to 19 nM (somatostatin, 5.6 nM), with the PEGylated analogs (1b and 2b) showing the lowest affinity to SSTR-2. All analogs except for the scrambled peptide also showed detectable activity against SSTR-4, but the affinity was poor (≥5.4 mM). None of the compounds exhibited detectable activity against SSTR-3 (data not shown).

Table 2: The SSTR-binding affinity of the Tyr^3^-octreotate analogs

Compound | Half-Maximal Effective Concentration
Compound | SSTR-2 | SSTR-4
Somatostatin | 5.6 nM | 3.8 nM
^19^F-FET-G-PEG-TOCA | 19.0 nM | >10 mM
^19^F-FETE-PEG-TOCA | 12.0 nM | >10 mM
^19^F-FET-βAG-TOCA | 4.7 nM | 8.6 mM
^19^F-FET-G-TOCA | 6.9 nM | 5.4 mM
^19^F-FETE-TOCA | 4.1 nM | 6.5 mM
^19^F-FET-βAG-[W-c-(CTFTYC)K] | 220 nM | ND

ND, not determined.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21852355)]

Leyton et al. examined the in vivo plasma stability of ^18^F-FET-βAG-TOCA at 30 min after tail vein injection (~3.7 MBq (0.1 mCi)) into BALB/c nu/nu mice (2). The radiochromatograms of the mouse plasma showed no metabolites of ^18^F-FET-βAG-TOCA.

Dynamic PET scans were performed over 60 min after tail vein injection of 3.0–3.7 MBq (0.08–0.10 mCi) of different radiolabeled analogs in mice bearing SSTR-2–expressing AR42J tumors (n = 3–6 mice/agent) (2). The radiotracer uptake for each organ was normalized to injected dose and expressed as percentage of injected activity per milliliter of tissue (% ID/mL) (Table 3). Tissues were collected after the 60-min PET scan, and the radioactivity was accounted and expressed as a percentage injected dose per gram tissue (% ID/g) (Table 3) (2). The results were compared with the data obtained with clinical radiotracer ^68^Ga-DOTATATE and recently synthesized ^18^F-AIF-NOTA-OC.

The tumor uptake for all radiotracers was characterized by a rapid increase over the entire scanning period of 60 min. ^18^F-FET-G-TOCA had the highest tumor uptake, followed by ^18^F-FET-βAG-TOCA. With respect to tumor uptake, tumor/muscle (T/M) ratio, and tumor/blood (T/B) ratio, these tracers were superior to the clinical radiotracer ^68^Ga-DOTATATE and comparable to the recently synthesized ^18^F-AIF-NOTA-OC (statistical data were not reported) (Table 3). PEG linkers conjugated to ^18^F-FET-G-PEG-TOCA and ^18^F-FETE-PEG-TOCA reduced tumor uptake but increased T/M and T/B ratios. Nonspecific uptake in the liver was, in general, low (<7% ID/mL), with ^18^F-FET-βAG-TOCA showing the lowest liver uptake and ^18^F-FET-G-TOCA and ^18^F-FETE-PEG-TOCA showing the highest liver uptake. The kinetic profiles of the analogs in the kidney, which also expresses SSTR-2, were different from those in tumors, showing the highest uptake for ^18^F-FET-βAG-TOCA and ^18^F-FET-G-TOCA. The mean muscle uptake was <3% ID/mL for all radiotracers. Radiotracer uptake in the bone was low for all analogs, indicating little or no defluorination. In contrast, no radiotracer localization was seen in tumors for the scrambled peptide ^18^F-FET-βAG-[W-c-(CTFTYC)K]; in this case, tracer localization was seen mainly in the brain, urine, liver, and intestines (data not shown). Uptake in the liver was higher with ^18^F-FET-βAG-[W-c-(CTFTYC)K] than with ^18^F-FET-βAG-TOCA.

Table 3: Biodistribution of octreotate analogs

Octreotate Analogs | PET-Tumor* | Tumor | Muscle | Blood | T/M | T/B
^18^F-FET-G-PEG-TOCA | 5.36 ± 0.45 | 8.29 ± 1.42 | 0.14 ± 0.10 | 0.35 ± 0.22 | 59.21 | 23.69
^18^F-FETE-PEG-TOCA | 5.14 ± 0.40 | 4.51 ± 1.52 | 0.19 ± 0.05 | 0.21 ± 0.03 | 23.74 | 21.48
^18^F-FET-G-TOCA | 11.00 ± 1.49 | 17.05 ± 2.77 | 1.49 ± 0.59 | 1.61 ± 0.65 | 11.44 | 10.59
^18^F-FETE-TOCA | 6.11 ± 1.46 | 9.79 ± 2.57 | 0.79 ± 0.23 | 1.05 ± 0.32 | 12.39 | 9.32
^18^F-FET-βAG-TOCA | 8.23 ± 2.02 | 11.58 ± 0.67 | 0.48 ± 0.21 | 0.86 ± 0.27 | 24.12 | 13.47
Blocking study** | 6.24 ± 0.64 | 3.93 ± 0.99 | 1.39 ± 0.51 | 0.63 ± 0.54 | 2.83 | 6.24
^18^F-FET-βAG-[W-c-(CTFTYC)K | 0.10 ± 0.05 | 0.22 ± 0.12 | 0.34 ± 0.30 | 0.20 ± 0.01 | 0.65 | 1.10
^18^F-AIF-NOTA-OC | 6.43 ± 0.85 | 12.73 ± 2.05 | 0.34 ± 0.10 | 0.55 ± 0.24 | 37.44 | 23.15
^68^Ga-DOTATATE | 2.75 ± 0.11 | 1.37 ± 0.16 | 0.60 ± 0.08 | 2.45 ± 0.56 | 2.28 | 0.56

*Data were from PET scans at 60 min after injection.

**Blocking study data for ^18^F-FET-βAG-TOCA.

Blocking studies were performed for ^18^F-FET-βAG-TOCA with injection of 10 mg/kg body weight of unlabeled octreotide in mice 10 min before injection of ^18^F-FET-βAG-TOCA (Table 3) (2). This injected dose of octreotide was ~100-fold higher than the equivalent dose of unlabeled ^18^F-FET-βAG-TOCA. Pre-injection of octreotide resulted in a two-fold (by direct counting) lower uptake of ^18^F-FET-βAG-TOCA in AR42J xenografts and higher reductions in T/M and T/B ratios (Table 3). After blocking with unlabeled octreotide, muscle radioactivity increased; kidney radioactivity decreased (early time points only) but subsequently increased; urine radioactivity decreased. The specificity of ^18^F-FET-βAG-TOCA uptake was also indicated by the low uptake in HCT116 xenografts (low SSTR expression), showing 2.42 ± 0.35% ID/mL in the tumor at 60 min (PET scanning data) and 0.52 ± 0.39, 0.58 ± 0.45, and 1.19 ± 0.89% ID/g in the tumor, muscle, and blood, respectively, after 60 min (ex vivo counting) (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed]

No references are currently available.

## References

1 Iddon L., et al. (2011). Synthesis and in vitro evaluation of [18F]fluoroethyl triazole labelled [Tyr3]octreotate analogues using click chemistry. Bioorg Med Chem Lett.
2 Leyton J., et al. (2011). Targeting somatostatin receptors: preclinical evaluation of novel 18F-fluoroethyltriazole-Tyr3-octreotate analogs for PET. J Nucl Med.
3 Modlin I.M., et al. (2008). Gastroenteropancreatic neuroendocrine tumours. Lancet Oncol.
4 Miederer M., Weber M.M., Fottner C. (2010). Molecular imaging of gastroenteropancreatic neuroendocrine tumors. Gastroenterol Clin North Am.
5 Krenning E.P., et al. (1989). Localisation of endocrine-related tumours with radioiodinated analogue of somatostatin. Lancet.
6 Krenning E.P., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Teunissen J.J., et al. (2011). Nuclear medicine techniques for the imaging and treatment of neuroendocrine tumours. Endocr Relat Cancer.
8 Evans H.L., et al. (2012). Copper-free click--a promising tool for pre-targeted PET imaging. Chem Commun (Camb).
9 Hofmann M., et al. (2001). Biokinetics and imaging with the somatostatin receptor PET radioligand (68)Ga-DOTATOC: preliminary data. Eur J Nucl Med.
10 Meisetschlager G., et al. (2006). Gluc-Lys([18F]FP)-TOCA PET in patients with SSTR-positive tumors: biodistribution and diagnostic evaluation compared with [111In]DTPA-octreotide. J Nucl Med.